# Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(TDOPA)_3_-flower-like gold–Fe_3_O_4_ optical nanoparticles

Chemical name: | Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(TDOPA)_3_-flower-like gold–Fe_3_O_4_ optical nanoparticles
Abbreviated name: | FANPs
Synonym:
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Gold has not been used as an X-ray contrast agent in vivo. Gold has a higher atomic number and a higher absorption coefficient than iodine, providing 2.7-fold greater contrast/weight than iodine (4). Furthermore, imaging gold at 80–100 keV reduces interference from bone absorption and provides lower soft tissue absorption, which would reduce radiation to patients. Hainfeld et al. (4) used gold nanoparticles (AuNPs; 1.9 nm in diameter, ~50 kDa) as a computed tomography (CT) contrast agent in mice; these experiments showed enhanced CT contrast of the vasculature, kidneys, and tumors in mice. However, plasma proteins in blood adsorb onto the surface of bare AuNPs, which produces large aggregates (5) that may result in altered pharmacokinetics and biodistribution of AuNPs (6). Polyethylene glycol (PEG) is found to minimize nonspecific adsorption of proteins onto NPs and to reduce their uptake by the liver (6). PEG-AuNPs have been being studied as cancer CT imaging and photothermal agents (7).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (8-11). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (12). The peptide Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-NH_2_ was found to be a MMP substrate and is cleaved between the Leu and Gly residues. Lee et al. (13) used this sequence with a Cy5.5 NIR dye molecule to attach to AuNPs to form fluorescence-quenched nanoparticles (Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-AuNPs (Cy5.5-MMP-AuNPs or GANPs). The Cy5.5 molecules are in close proximity, resulting in fluorescence quenching because of efficient fluorescence resonance energy transfer to Au. NIR fluorescence signal will increase when the Leu-Gly bond is cleaved by MMPs, releasing Cy5.5-containing fragments. Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm, an emission maximum at 694 nm, and a high extinction coefficient of 250,000 M−^1^cm−^1^. Cy5.5-MMP-AuNPs are being developed for NIR fluorescence imaging of MMPs expressed in tumors, atherosclerosis, myocardial infarction, and other diseases. Xie et al. (14) replaced the AuNP with Au-Fe_3_O_4_, a composite NP shaped like a flower, to induce a fluorescently quenched state to the overall nanostructure. There were three iron oxide “petals” on each AuNP. The MMP peptide was covalently linked to an anchoring unit, Lys-tridihydrophenylalanine (Lys-TDOPA) on the surface of the iron oxide NP. The gold surface was passivated with a thiolated PEG (SH-PEG_5000_). Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_-flower-like gold–Fe_3_O_4_ optical NPs (FANPs) have been evaluated for imaging protease expression in vivo.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D), gold nanoparticles (http://www.ncbi.nlm.nih.gov/books?term=gold%20nanoparticles%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (MMP13 (http://www.ncbi.nlm.nih.gov/gene/4322))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP13 (http://www.ncbi.nlm.nih.gov/omim/600108))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle)]

Xie et al. (14) prepared FANPs in multiple steps. First, Fe_3_O_4_ was allowed to seed onto the surface of AuNPs (8 nm) via pyrolysis using Fe(CO)_5_ for 10 min at 220°C to form flower-like gold–Fe_3_O_4_ NPs. Second, Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_ was prepared using standard solid-phase peptide synthesis. Cy5.5 was conjugated to the N-terminus of Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_ to produce Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_. Third, 0.4 mg Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_ and 25 mg SH-PEG_5000_ in 0.9 ml DMSO was added to 2 ml gold–Fe_3_O_4_ NPs (27 mg) in CHCl_3_. The mixture was incubated at room temperature for ~18 h. FANPs were collected by centrifugation. The iron oxide “petals” had a diameter of 13.4 ± 3.5 nm. The overall diameter of FANPs was 40.0 ± 4.3 nm, as determined with dynamic light scattering. There were 152 ± 12 molecules of Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_ per FANP. The quenching efficiency of a single FANP was estimated to be >95%. FANPs were stable in phosphate-buffered saline, 10 mM dithiothreitol (DTT) solution, and medium containing fetal bovine serum after 2–3 h of incubation at 37°C. DTT did not cleave the peptides off the FANPs.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle%20and%20in%20vitro)]

Xie et al. (14) showed that FANPs (14 nM) was activated by MMP-13 in a time-dependent manner with Leu-Gly bond cleavage. There was a 17-fold increase in NIR fluorescence signal after 420 min of incubation with MMP-13 (3 µg/ml) over the control without MMP-13. Co-incubation with a broad-spectrum MMP inhibitor (1 µM) markedly reduced NIR fluorescence signal from MMP-13 to near background level.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle%20and%20rodentia)]

Xie et al. (14) performed biodistribution studies of FANPs and GANPs (150 nmol Cy5.5/kg) intravenously injected in nude mice (the number of mice per group used was not reported) bearing human SCC7 squamous cell carcinoma cell line (MMP-13–positive). Whole-body optical imaging was performed at 30, 60, 120, and 240 min after injection. In the FANP group, good NIR fluorescence signal was visualized at 30 min, and the signal increased by approximately three-fold at 240 min as compared with the signal at 30 min. The tumor signals were estimated to be 415 × 10^6^, 855 × 10^6^, 1,165 × 10^6^, and 1,523 × 10^6^ photon·cm−^2^·s−^1^ at 30, 60, 120, and 240 min, respectively. In contrast, the GANP group showed little signal in the tumors at these time points with 47 × 10^6^ photon·cm−^2^·s−^1^ at 240 min. Intratumoral injection of MMP-13 inhibitor (1 mg/kg) 30 min before FANP injection completely blocked the signals in the tumors to <28 × 10^6^ photon·cm−^2^·s−^1^ at these time points. Ex vivo imaging of the tumors and major organs was performed at 240 min after injection. The signals from the tumors were correlated with those observed in the in vivo imaging. The tumor signals from the FANP group were approximately nine-fold and four-fold higher than those observed in the FANP+MMP inhibitor and GANP groups, respectively. The signals in the liver were ~20% higher than the tumor signals from the FANP group. The signals in the spleen, kidneys, and lung were moderate (lower than the tumors), with low signals in the muscle, heart, bone, and blood. Histo-immunological staining of tumor sections revealed a strong expression of MMP-13 in the tumors, with co-localization of NIR fluorescence signals in the FANP group. In the FANP+MMP inhibitor group, there was a co-localization of the FANP in the tumors but without Cy5.5 NIF signals because the MMP inhibitor inhibited the cleavage of Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-(Lys-TDOPA)_3_ by MMPs from the FANPs. The accumulation of FANPs in tumors was likely mediated by the enhanced permeability and retention effects.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Flower-like%20gold%20iron%20oxide%20nanoparticle%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
5 Zhang F., Skoda M.W., Jacobs R.M., Zorn S., Martin R.A., Martin C.M., Clark G.F., Goerigk G., Schreiber F. (2007). Gold nanoparticles decorated with oligo(ethylene glycol) thiols: protein resistance and colloidal stability. J Phys Chem A.
6 Otsuka H., Nagasaki Y., Kataoka K. (2003). PEGylated nanoparticles for biological and pharmaceutical applications. Adv Drug Deliv Rev.
7 Cai Q.Y., Kim S.H., Choi K.S., Kim S.Y., Byun S.J., Kim K.W., Park S.H., Juhng S.K., Yoon K.H. (2007). Colloidal gold nanoparticles as a blood-pool contrast agent for X-ray computed tomography in mice. Invest Radiol.
8 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
9 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
10 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
11 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
12 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
13 Lee S., Cha E.J., Park K., Lee S.Y., Hong J.K., Sun I.C., Kim S.Y., Choi K., Kwon I.C., Kim K., Ahn C.H. (2008). A near-infrared-fluorescence-quenched gold-nanoparticle imaging probe for in vivo drug screening and protease activity determination. Angew Chem Int Ed Engl.
14 Xie J., Zhang F., Aronova M., Zhu L., Lin X., Quan Q., Liu G., Zhang G., Choi K.Y., Kim K., Sun X., Lee S., Sun S., Leapman R., Chen X. (2011). Manipulating the power of an additional phase: a flower-like Au-Fe3O4 optical nanosensor for imaging protease expressions in vivo. ACS Nano.